# ^67/68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-1,2-diaminoethane-γ-folate

Chemical name: | ^67/68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-1,2-diaminoethane-γ-folate
Abbreviated name: | ^67/68^Ga-P3026
Synonym:
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET); single-photon emission computed tomography (SPECT)
Source of signal: | ^67/68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3026)]

Folic acid (folate) is a water-soluble B vitamin (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher-affinity (dissociation constant (K_d_) = 0.5 nM) receptor that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells have been found to overexpress folate-binding protein (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the corresponding normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have been also found to have the folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate, ^99m^Tc-EC-folate, and [^18^F]FBA-folate) have been studied in tumor imaging (4-8). Deferoxamine (DF), a chelating agent, was conjugated to folic acid forming a mixture of two isomers, DF-α-folate and DF-γ-folate. Only the DF-γ-folate isomer was able to displace [^3^H]folic acid from its receptors with a 50% inhibition concentration similar to that of folic acid (2.5 nM versus 2.4 nM) (9). ^68/67/66^Ga-γ-DF-folate is being developed as an imaging agent for the detection of folate receptors in vivo with either positron emission tomography (PET) or single-photon emission computed tomography (SPECT). In this chapter, Fani et al. (10) prepared a γ-folate conjugate with tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) and 1,2-diaminoethane as a spacer to form P3026, which was labeled with ^67/68^Ga for detection of folate receptors.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3026%20and%20synthesis)]

Fani et al. (10) coupled P3026 (10 nmol) with 74 MBq (2 mCi) ^67^GaCl_3_ in acetate buffer (pH 5) for 30 min at 95°C to yield ^67^Ga-P3026 with >92% radiochemical purity. Radiochemical yields exceeded 95% with a specific activity of 7 MBq/nmol (0.19 mCi/nmol). ^68^Ga-P3026 was similarly radiolabeled for 10 min at 95°C with a specific activity of 9 MBq/nmol (0.24 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3026%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB cell line has putative folate receptors as determined with ^67^Ga-P3026 saturation binding studies at 4°C (10). ^67^Ga-P3026 showed a K_d_ (affinity constant) of 4.65 ± 0.82 nM and a B_max_ (receptor density) of 10.65 ± 0.45 nM. There were ~6.4 × 10^6^ folate binding sites per KB cell. ^67^Ga-P3026 (2.5 nM) was rapidly associated with KB cells at 37°C with 60% of incubation dose (ID) at 30 min and 80% ID at 4 h. Approximately 16% ID of ^67^Ga-P3026 was internalized at 4 h. Excess folate blocked the cell-associated radioactivity to <0.5% ID. Approximately 80% of radioactivity was retained in the cells after 4 h incubation in fresh medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3026%20and%20rodentia)]

Fani et al. (10) performed ex vivo biodistribution studies of 1.5 MBq (0.041 mCi, 0.4 nmol) ^67^Ga-P3026 in nude mice (n = 4–7/group) bearing KB and HT1080 (low folate receptor expression) tumor xenografts. Accumulation of ^67^Ga-P3026 in the KB tumors was 11.8 ± 2.8, 10.6 ± 2.1, and 14.3 ± 4.1% ID/g at 1, 2, and 4 h after injection, respectively. The accumulation in the HT1080 tumors was 1.0%–1.5% ID/g at these time points. The organ with the highest accumulation at 4 h after injection was the kidney (103.0% ID/g), followed by the pancreas (3.3% ID/g), adrenal (3.2% ID/g), heart (2.5% ID/g), pituitary (2.3% ID/g), and liver (2.1% ID/g). The accumulation in the blood was low (<0.5% ID/g). The tumor/blood ratios were 36, 50, and 70 at 1, 2, and 4 h, respectively. Pretreatment with excess folate (40 nmol, 5 min before injection) reduced the radioactivity accumulation by >90% in the tumors and kidney at 4 h after injection.

The whole-body distribution was also assessed with PET imaging at 1 h after injection of 4 MBq (0.11 mCi) ^68^Ga-P3026 (0.4 nmol). The highest activity concentrations were visualized in the KB tumors and kidneys, whereas the HT1080 tumors were barely visible. The accumulation of ^68^Ga-P3026 in the KB tumors and kidneys was blocked by pre-injection of excess folic acid (40 nmol, 5 min).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3026%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3026%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3026%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.
9 Wang S., Lee R.J., Mathias C.J., Green M.A., Low P.S. (1996). Synthesis, purification, and tumor cell uptake of 67Ga-deferoxamine--folate, a potential radiopharmaceutical for tumor imaging. Bioconjug Chem.
10 Fani M., Wang X., Nicolas G., Medina C., Raynal I., Port M., Maecke H.R. (2011). Development of new folate-based PET radiotracers: preclinical evaluation of Ga-DOTA-folate conjugates. Eur J Nucl Med Mol Imaging.